# IRDye 700DX-Labeled annexin V

Chemical name: | IRDye 700DX-Labeled annexin V
Abbreviated name: | NIR700-Annexin V
Synonym:
Agent Category: | Ligand
Target: | Phosphatidylserine
Target Category: | Phospholipid
Method of detection: | Near-infrared (NIR) imaging
Source of signal / contrast: | IRDye 700DX
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Annexin+imaging+probes)

The epidermal growth factor (EGF) receptor (EGFR) that mediates its activity (cell development, proliferation and migration etc.) through an intracellular kinase (TK) is overexpressed in several different types of cancers, including that of the colorectal area. Because of its cancer-promoting activity, the EGFR has been targeted to treat the malignancies with monoclonal antibodies (mAbs) directed toward its extracellular domain, with inhibitors against the TK, or with a combination of the two treatment methods (1-3). Although the United States Food and Drug Administration has approved these therapies for cancers, the response rate to a single agent treatment, particularly for colorectal cancer (CRC), is low, and it is difficult to predict which patient is likely to respond to the therapy (4, 5). Often biopsies have to be performed on the patients to predict possible cancer treatment outcomes, with mAbs targeting the EGFR or with drugs directed toward the intracellular TK, and no noninvasive biomarkers are available to determine the prognosis or to monitor therapy response (5). Biopsies, however, carry a risk of infection for the patient, the tissue must be examined microscopically by a specialist for diagnosis, and sampling of a small fraction of the tumor can result in false negative observations.

Manning et al. developed IRDye 700DX (http://www.licor.com/bio/IRDye/PL-IRDyes700DX.jsp)-labeled annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez) (NIR700DX-Annexin V), an apoptosis biomarker, in an effort to develop a noninvasive, near-infrared optical imaging technique to determine the efficacy of cetuximab (http://packageinserts.bms.com/pi/pi_erbitux.pdf) in mice bearing human CRC cell line xenograft tumors (4). The investigators also used IRDye 800CW-labeled EGF (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=IRDye800CW-EGF) (NIR800-EGF) to assess the inhibition of cetuximab signaling in the tumor cells, and they used 3’-[^18^F]fluoro-3’-deoxythymidine (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Fluorothymidine18F) ([^18^F]FLT) with positron emission tomography (PET) to determine cell proliferation in the tumors.

### Other sources of information

Cetuximab (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Cetuximab+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) and annexin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Annexin+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) chapters in MICAD.

Drug information (http://www.accessdata.fda.gov/drugsatfda_docs/label/2004/125084lbl.pdf) regarding cetuximab.

Clinical trials (http://clinicaltrials.gov/ct2/results?term=annexins) related to annexin.

Clinical trials (http://clinicaltrials.gov/ct2/results?term=egfr) related to EGFR.

Annexin in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=annexin).

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=egfr%20gene).

Drug and other information regarding annexin V – FDA (http://google2.fda.gov/search?q=Annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*).

Drug and other information regarding EGFR – FDA (http://google2.fda.gov/search?q=EGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=IRDye%20700DX-annexin%20V%20synthesis&cmd=DetailsSearch)]

The synthesis of NIR700DX-Annexin V has been discussed in detail by Manning et al. (4). A similar method was used to obtain NIR800-EGF (4). Purity of the two conjugates was assessed with a chromatographic method (not specified), and the dye/protein ratio was routinely 1:1 as determined with spectrophotometry. The storage conditions and stability of the labeled proteins were not reported.

The synthesis of [^18^F]FLT was described by Manning et al. (4). The radiochemical identity, purity, and specific activity of the tracer were determined with analytical high-performance liquid chromatography. The average radiochemical purity of [^18^F]FLT was reported to be 98.3% with a specific activity of 128.88 TBq/mmol (3,480 Ci/mmol). The storage conditions and stability of the labeled compound were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=IRDye%20700DX-labeled%20annexin%20V%20in%20vitro&cmd=DetailsSearch)]

The human colorectal cell line DiFi (6), which expresses high levels of EGFR, was used to characterize the in vitro properties of NIR800-EGF and NIR700DX-Annexin V (4). The DiFi cells were shown with fluorescence microscopy to bind and internalize NIR800-EGF. These observations were confirmed using A431 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1555&Template=cellBiology) that also express high levels of the EGFR. The binding of NIR800-EGF to both cell types was reduced nearly to background levels in the presence of unlabeled EGF, indicating that the probe bound specifically to the EGFR. Treatment of the DiFi cells with cetuximab was shown to induce apoptosis (as measured by caspase-3/7 activity) and reduce cell proliferation (as determined with cell cycle analysis using propidium iodide (Ki) and flow cytometry) in a concentration-dependent manner.

In another study, DiFi cells treated with increasing concentrations of cetuximab were exposed to NIR700DX-annexin V, and uptake of the probe was shown to correlate with the amount of mAb used to treat the cells (4).

With results from these studies, the investigators concluded that NIR800-EGF and NIR700DX-annexin V could be used as reporter probes to determine the binding of cetuximab to the EGFR (because the mAb would compete with EGF for binding to the EGFR) and to determine the degree of apoptosis induced by cetuximab in the cells under in vitro conditions (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Using nude mice respectively bearing xenograft tumors derived from HCT-116 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-247&Template=cellBiology) (cetuximab-resistant cells with moderate EGFR expression; n = 16 animals), DiFi (high EGFR expression; n = 14 animals), and SW620 (EGFR-negative controls; n = 9 animals) cells, NIR800-EGF imaging was shown to quantify the level of EGFR expressed on the various tumor cells (4). This quantification was confirmed with EGFR immunoreactivity in the tumor tissues.

To investigate the in vivo uptake and clearance properties of NIR700DX-Annexin V, a group of mice (n = 8) bearing DiFi xenograft tumors was treated with cetuximab (three treatments of 40 mg/kg every 3 days) followed by intravenous administration of the annexin probe by retro-orbital injection (4). Imaging was performed on the mice over a period of 40 h after injection of the probe. Control animals received the probe injection without cetuximab pretreatment. Minimal uptake of NIR700DX-Annexin V was observed in the tumors of control animals, although some accumulation of the probe was observed in the kidneys. A significantly (P < 0.0001) higher retention of the annexin probe was reported in tumors of the cetuximab-treated animals, indicating that the probe was useful in the quantification of apoptosis/necrosis. Apoptosis of tumor cells from the cetuximab-treated animals was confirmed with a histological analysis of the caspase-3 activity.

The cetuximab inhibition of TK signaling (initiated by the activation of EGFR) and induction of apoptosis in the tumors was assessed by imaging the uptake of NIR800-EGF and NIR700DX-Annexin V, respectively, in mice bearing DiFi (n = 26 animals) or HCT-116 (n = 16 animals) cell xenograft tumors (4). The proliferation of tumor cells in the two groups of animals was determined with PET imaging using [^18^F]FLT (4). Control animals were not pretreated with cetuximab. Compared with controls, tumors of the cetuximab-treated animals showed a significantly (P < 0.0001) reduced accumulation of NIR800-EGF with a corresponding increase (P = 0.0006) in the signal from NIR700DX-Annexin V. However, little difference was noted in the tumor uptake of [^18^F]FLT in the cetuximab-treated or untreated animals, indicating that cetuximab did not reduce cell proliferation in these tissues. The induction of apoptosis in the cetuximab-treated tumor cells was confirmed by significantly elevated caspase-3 histological staining compared with controls, confirming the observations made with NIR700-Annexin V imaging that cetuximab induces apoptosis in tumor cells. In addition, Ki-67 staining of the cetuximab-treated and untreated tumor cells as a measure of proliferation showed there was little difference in staining between the two groups, corroborating the observation made earlier with [^18^F]FLT PET imaging. Compared with the DiFi cell tumors of the cetuximab-treated animals, the HCT-116 cell xenograft tumors showed little or no change in uptake of the NIR800-EGF, NIR700DX-annexin, or the PET imaging probes, and these observations were verified by histological methods mentioned above. These observations indicated that concomitant use of the NIR800-EGF, NIR700DX-Annexin V, and [^18^F]FLT probes could distinguish cetuximab-sensitive tumors from cetuximab-insensitive tumors.

From these results the investigators concluded that the imaging methods performed in this study to determine the efficacy of EGFR-targeted therapies (e.g., the use of mAbs against the receptor) could be useful for the preclinical evaluation of new cancer treatment regimens in mice (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=IRDye%20700DX%20annexin%20V%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=IRDye%20700DX%20annexin%20V%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some studies were supported by National Cancer Institute grants CA 46413, K25 CA127349, U24 CA126588, and 1S10 RR17858. Studies were also supported by National Institutes of Health grants T32 EB03817 and T32 EB003817.

## References

1 Hopper-Borge E.A., Nasto R.E., Ratushny V., Weiner L.M., Golemis E.A., Astsaturov I. (2009). Mechanisms of tumor resistance to EGFR-targeted therapies. Expert Opin Ther Targets.
2 Siena S., Sartore-Bianchi A., Di Nicolantonio F., Balfour J., Bardelli A. (2009). Biomarkers predicting clinical outcome of epidermal growth factor receptor-targeted therapy in metastatic colorectal cancer. J Natl Cancer Inst.
3 Baselga J., Arteaga C.L. (2005). Critical update and emerging trends in epidermal growth factor receptor targeting in cancer. J Clin Oncol.
4 Manning H.C., Merchant N.B., Foutch A.C., Virostko J.M., Wyatt S.K., Shah C., McKinley E.T., Xie J., Mutic N.J., Washington M.K., LaFleur B., Tantawy M.N., Peterson T.E., Ansari M.S., Baldwin R.M., Rothenberg M.L., Bornhop D.J., Gore J.C., Coffey R.J. (2008). Molecular imaging of therapeutic response to epidermal growth factor receptor blockade in colorectal cancer. Clin Cancer Res.
5 Walther A., Johnstone E., Swanton C., Midgley R., Tomlinson I., Kerr D. (2009). Genetic prognostic and predictive markers in colorectal cancer. Nat Rev Cancer.
6 Olive M., Untawale S., Coffey R.J., Siciliano M.J., Wildrick D.M., Fritsche H., Pathak S., Cherry L.M., Blick M., Lointier P., et al. (1993). Characterization of the DiFi rectal carcinoma cell line derived from a familial adenomatous polyposis patient. In Vitro Cell Dev Biol.